# 4-Hydroxy-, 5-hydroxy-, and 7-hydroxy- analogs of 6-hydroxy-2-(4’-[^11^C]methylaminophenyl)-1,3-benzothiazole

Chemical name: | 4-Hydroxy-, 5-hydroxy-, and 7-hydroxy- analogs of 6-hydroxy-2-(4’-[^11^C]methylaminophenyl)-1,3-benzothiazole | [image]
Abbreviated name: | [^11^C]6a, [^11^C]6b, and [^11^C]6c | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | β-Amyloid plaques (Aβ) | [image]
Target Category: | Protein | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^11^C | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^11^C]6a, [^11^C]6b and [^11^C]6c.

## Background

[PubMed] (http://www.ncbi.nlm.nih.gov/pubmed?term=amyloid%20imaging%20agents&cmd=DetailsSearch)

Development of Alzheimer’s disease (AD) has been attributed to neurodegeneration as a result of the neuronal overexpression, secretion, and extracellular deposition of the neurotoxic amyloid-β (Aβ) fragment of the Aβ protein precursor in the brain (1). In addition, the AD brain neurons are known to form and deposit neurofibrillary tangles in the cytoplasm (2). No specific treatment for AD is currently available, and researchers and clinicians are increasingly focused on developing ways to either prevent or delay the formation of Aβ plaques in the brain of AD patients (3). In addition, several hundred clinical trials (http://clinicaltrials.gov/ct2/results?term=Alzheimer%E2%80%99s+disease+) approved by the United States Food and Drug Administration have been completed or are in progress to develop drugs for the prevention, onset delay, or treatment of AD. Early detection of Aβ plaques by non-invasive techniques such as positron emission tomography (PET) is often used to identify individuals who are prone to get the disease and to monitor the efficacy of drugs used to treat or delay onset of the disease (4). Although several immunohistochemical fluorescent stains and an antibody directed against the Aβ have been used to detect the plaques in the brain of AD patients, this information can be obtained only during postmortem (5). Hence, the development and evaluation of a suitable agent for the non-invasive detection of Aβ plaques during early onset or to monitor progression and treatment of the disease is an ongoing task.

Many radiolabeled tracers have been developed and evaluated under preclinical conditions, but among these only the ^11^C-labeled Pittsburgh compound B (6-hydroxy-2-(4’-N-[^11^C]methylaminophenyl)-1,3-benzothiazole ([^11^C]PIB (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=PIB11C))) is the most commonly used agent for the PET imaging of Aβ plaques (2, 4, 5). Clinical evaluation of ^18^F-labeled PIB derivatives for the detection of Aβ plaques is an ongoing process, and efforts are under way to develop other imaging agents that could be superior to PIB. In this regard, Serdons et al. (2) synthesized three ^11^C-labeled structural isomers of PIB with the hydroxyl group at position 4, 5, or 7 (designated as [^11^C]6a, [^11^C]6b, and [^11^C]6c, respectively), compared to the position 6 hydroxyl group in PIB, and investigated the binding of these labeled compounds to Aβ plaques in mouse and human AD brain sections. The biodistribution of these tracers, particularly in the brain, was also compared to that of [^11^C]PIB in normal mice.

### Other sources of information regarding human β amyloid protein

β Amyloid plaques in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Beta%20amyloid%20plaques) (Online Mendelian Inheritance in Man).

Human β amyloid protein (http://www.ncbi.nlm.nih.gov/protein/P05067.3?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=351&log$=databasead1&logdbfrom=nuccore) sequence.

Alzheimer’s disease in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Alzheimer%E2%80%99s%20disease%20).

Alzheimer’s disease in Genome Wide Association Studies (http://www.genome.gov/gwastudies/index.cfm?#searchForm) database.

FDA-approved treatments (http://www.alz.org/national/documents/topicsheet_treatments.pdf) for Alzheimer’s disease (from Alzheimer’s Association web site; www.alz.org).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=hydroxy-2-%284-methylaminophenyl%29-1%2C3-benzothiazole%20synthesis&cmd=DetailsSearch)]

The synthesis processes of [^11^C]6a (4-hydroxy-2-(4’-methylaminophenyl)-1,3-benzothiazole), [^11^C]6b (5-hydroxy-2-(4’-methylaminophenyl)-1,3-benzothiazole), and [^11^C]6c (7-hydroxy-2-(4’-methylaminophenyl)-1,3-benzothiazole) were described in detail by Serdons et al. (2). The identity of the labeled compounds was confirmed with radio-high-performance liquid chromatography and radio-mass spectrometry. The specific activity, radiochemical purity, and stability of the labeled compounds were not reported. The radiochemical yield of [^11^C]6a was not reported, but the radiochemical yields for [^11^C]6b and [^11^C]6c were reported to be 5% and 7%, respectively (not decay-corrected).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=hydroxy-2-%284-methylaminophenyl%29-1%2C3-benzothiazole%20in%20vitro%20studies&cmd=DetailsSearch)]

Using an [^125^I]IMPY competition assay, Serdons et al. determined the affinity of unlabeled 6a, 6b, and 6c for Aβ fibrils in human AD brain homogenates (2). The inhibition constant values of 6a, 6b, and 6c were reported to be 18.8 ± 3.8, 11.5 ± 3.0, and 11.2 ± 0.5 nM compared to that of 2.8 ± 0.5 for nonradioactive PIB.

The binding of nonradioactive 6a, 6b, and 6c to Aβ plaques in brain sections obtained from transgenic AD mice and the brain of an AD patient was confirmed with fluorescent microscopy and in Aβ antibody co-localization studies, and it has been described by Serdons et al. (2).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=hydroxy-2-%284-methylaminophenyl%29-1%2C3-benzothiazole%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^11^C]6a, [^11^C]6b, and [^11^C]6c was compared to that of [^11^C]PIB in normal mice (2). Groups of 4 animals/time point were injected with the different labeled compounds through the tail vein, and the mice were euthanized at 2 min and 60 min postinjection (p.i.). Various organs (kidneys, liver, intestine, cerebrum, cerebellum, and blood) were removed from the euthanized animals, and radioactivity accumulated in the different tissues was determined. Details of label uptake by the various tissues are presented in Tables 2–5 of Serdons et al. (2). Data were presented as a percentage of injected dose (% ID)/gram tissue (% ID/g). At 2 min p.i., [^11^C]6a, [^11^C]6b, and [^11^C]6c had uptake values similar to the parent compound. With [^11^C]6a, a higher amount of radioactivity was present in the cerebrum (3.8 ± 0.9% ID/g) than in the cerebellum (2.7 ± 2.1% ID/g), and the accumulated radioactivity was similar to that observed with [^11^C]PIB (3.6 ± 1.4% ID/g in cerebrum and 1.6 ± 0.1% ID/g in cerebellum). However, with [^11^C]6b and [^11^C]6c at the same time point, an equal amount of label was found to be distributed in the cerebrum (3–4%ID/g) and the cerebellum (3–4%ID/g) of the animals. At 60 min p.i., the washout rates of [^11^C]6b (0.09 ± 0.02% ID/g in cerebrum and 0.08 ± 0.07% ID/g in cerebellum) and [^11^C]6c (0.16 ± 0.03% ID/g in cerebrum and 0.10 ± 0.14% ID/g in cerebellum) from the brain were faster than washout of either [^11^C]6a (0.30 ± 0.30% ID/g in cerebrum and 0.60 ± 0.04%ID/g in cerebellum) or [^11^C]PIB (0.60 ± 0.20% ID/g in cerebrum and 0.30 ± 0.10% ID/g in cerebellum). The washout rate of [^11^C]6b from the brain areas was approximately eight-fold faster than that of [^11^C]PIB (by 60 min p.i.) compared to only a two-fold faster clearance rate noted with either [^11^C]6a or [^11^C]6c. The blood clearance ratios (% ID in blood at 2 min to % ID in blood at 60 min) of the label were 6, 12, and 8 for [^11^C]6a, [^11^C]6b, and [^11^C]6c, respectively, compared to a ratio of 3 for [^11^C]PIB. All of the labeled PIB analogs were excreted primarily through the hepatobiliary route, although some urinary clearance of the label was also observed.

According to Serdons et al. (2), a superior Aβ imaging agent should have a fast blood clearance with a rapid washout rate from the normal brain. On the basis of observations from this study, however, the investigators concluded that subtle structural changes introduced in PIB can have significant influence on the in vivo behavior of the compounds. Because none of the new PIB derivatives exhibited brain washout and blood clearance characteristics superior to [^11^C]PIB for the imaging of Aβ plaques, further evaluation of the analogs was suggested to be necessary before any of the ^11^C-labeled PIB derivatives could be used for the visualization of amyloid plaques in mouse or human brains with AD.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=11C%20labeled%20structural%20isomers%20of%20PIB%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=hydroxy-2-%284-methylaminophenyl%29-1%2C3-benzothiazole%20Non%20Human%20Primate%20studies&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=hydroxy-2-%284-methylaminophenyl%29-1%2C3-benzothiazole%20human%20studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Bissette G. (2009). Does Alzheimer's disease result from attempts at repair or protection after transient stress?. J Alzheimers Dis.
2 Serdons K., Verduyckt T., Vanderghinste D., Borghgraef P., Cleynhens J., Van Leuven F., Kung H., Bormans G., Verbruggen A. (2009). 11C-labelled PIB analogues as potential tracer agents for in vivo imaging of amyloid beta in Alzheimer's disease. Eur J Med Chem.
3 Sano M., Grossman H., Van Dyk K. (2008). Preventing Alzheimer's disease : separating fact from fiction. CNS Drugs.
4 Serdons K., Van Laere K., Janssen P., Kung H.F., Bormans G., Verbruggen A. (2009). Synthesis and evaluation of three 18F-labeled aminophenylbenzothiazoles as amyloid imaging agents. J Med Chem.
5 Serdons K., Terwinghe C., Vermaelen P., Van Laere K., Kung H., Mortelmans L., Bormans G., Verbruggen A. (2009). Synthesis and Evaluation of (18)F-Labeled 2-Phenylbenzothiazoles as Positron Emission Tomography Imaging Agents for Amyloid Plaques in Alzheimer's Disease. J Med Chem.